# N-(2-(2,5-dioxo-2,5-dihydro-1H-pyrrol-1-yl)ethyl)-4-[^18^F]-fluorobenzamide ([^18^F]FBEM) conjugated to EM3106B, an analog of glucagon-like peptide-1

Chemical name: | N-(2-(2,5-dioxo-2,5-dihydro-1H-pyrrol-1-yl)ethyl)-4-[^18^F]-fluorobenzamide ([^18^F]FBEM) conjugated to EM3106B, an analog of glucagon-like peptide-1
Abbreviated name: | [^18^F]FBEM-EM3106B
Synonym:
Agent Category: | Peptide
Target: | Glucagon-like peptide-1 receptor (GLP-1R)
Target Category: | Receptor
Method of detection: | Positron emission tomography (PET)
Source of signal / contrast: | ^18^F
Activation: | No
Studies: | - In vitro; - Rodents | Structure not available in PubChem (http://www.ncbi.nlm.nih.gov/pcsubstance).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=insulinoma&cmd=DetailsSearch)]

Pancreatic neuroendocrine tumors (PNET) are rare, are classified as nonfunctional or functional, and have been discussed in detail by Batcher et al. (1). Nonfunctional PNETs usually grow in size and eventually cause a mass effect in the organ, whereas functional tumors secrete one (or more) active hormones and are subclassified on the basis of the hormone secreted by the cells constituting the tumor (e.g., insulinomas (secrete insulin), glucagonomas (secrete glucagon), somatostatinomas (secrete somatostatin), etc.). Insulinomas are the most common PNETs observed in the clinic, and biochemical tests of patients with these tumors show that the individuals have fasting hypoglycemia (below normal glucose levels) along with hyperinsulinemia (elevated levels of insulin) (1). Complete surgical resection of the tumor is considered to be the most suitable treatment and cure for the patient (2). Most insulinomas are small and benign, and they exist as single lesions. Imaging techniques such as computed tomography (CT), magnetic resonance imaging (MRI), and endoscopic ultrasound (EUS) are often used to detect and determine the location of these tumors on the pancreas (3). However, the preoperative detection of these lesions with noninvasive imaging is difficult because the techniques are either unable to distinguish the tumor from the normal parenchymal tissue in the pancreas (e.g., CT), are expensive (e.g., MRI), invasive, and successful detection of the tumor is operator-dependent (e.g., EUS) (3, 4).

Investigators have shown that insulinomas characteristically express high levels of glucagon-like peptide 1 (GLP-1) receptors (GLP-1R), and radiolabeled GLP-1 analogs have been developed and evaluated for the detection of the PNETs (5). Although GLP-1 is the natural ligand for the GLP-1R, a major drawback of using this peptide to detect the lesions is that it is rapidly inactivated (half-life, ~2 min) by proteolytic enzymes while in circulation. As a consequence, investigators have used ^111^In- or ^99m^Tc-labeled exendin-4 or its analogs (exendin is a peptide of 39 amino acids that has a 54% homology with GLP-1, acts as an agonist of the GLP-1R, and is not inactivated by proteolytic enzymes) with single-photon emission computed tomography to detect insulinomas in Rip1Tag2 mice that have spontaneous insulinoma (6, 7) and in humans (4). Investigators have also used positron emission tomography (PET) with structural analogs of exendin-4 conjugated to N-(2-(2,5-dioxo-2,5-dihydro-1H-pyrrol-1-yl)ethyl)-4-[^18^F]-fluorobenzamide ([^18^F]FBEM) for labeling with ^18^F (e.g., [^18^F]FBEM-[Cys^0^]-exendin-4 and [^18^F]FBEM-[Cys^40^]-exendin-4; for structural details of these compounds, see Kiesewetter et al. (5)) to detect xenograft tumors that overexpress GLP-1R in mice (5). In a continued effort to develop GLP-1 analogs that are not degraded by proteolytic enzymes, investigators synthesized EM3106B, an analog of GLP-1 that contains lactam bridges between residues 18–22 and 30–34 of the peptide, has an unnatural amino acid (2-aminoisobutyric acid at position 8 (to prevent proteolytic degradation of the peptide)), and has a cysteine residue on the C-terminus to allow labeling with [^18^F]-FBEM. The GLP-1 analog was labeled with ^18^F (by coupling it with [^18^F]-FBEM), and the final labeled compound ([^18^F]FBEM-EM3106B) was evaluated for the detection of subcutaneous insulinomas in nude mice (6).

### Related Resource Links

Related chapters in MICAD (http://www.ncbi.nlm.nih.gov/books/?term=Exendin+AND+micad%5Bbook%5D&view=chapter&p%24a=&p%24l=PBooksLayout&p%24st=books)

Clinical trials (http://clinicaltrials.gov/ct2/results?term=GLP-1R) related to GLP-1R

Gene information (http://www.ncbi.nlm.nih.gov/gene/2740) regarding human GLP-1R (Gene ID: 2740)

Glucagon-like peptide 1 (http://omim.org/entry/138030) in Online Mendelian Inheritance in Man Database (OMIM)

Mouse GLP-1R (http://www.genome.jp/dbget-bin/www_bget?mmu:14652) in Kyoto Encyclopedia of Genes and Genomes Database (KEGG)

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=21800885%5Buid%5D&cmd=DetailsSearch)]

EM3106B was synthesized with a procedure detailed by Murage et al. (8). The radiochemical synthesis of [^18^F]FBEM has been discussed elsewhere (9). The radiochemical yield of [^18^F]FBEM was reported to be 17.3 ± 7.1% at ~95 min. Specific activities for three batches of the labeled compound were 181.3 GBq/μmol (4.88 Ci/μmol), 251.6 GBq/μmol (6.79 Ci/μmol), and 351.5 Gbq/μmol (9.49 Ci/μmol) at the end of bombardment (EOB) (9).

[^18^F]FBEM-EM3106B was produced as described by Gao et al. (7). The radiochemical yield of the labeled product (synthesis time 60 min) on the basis of ^18^F-FBEM was 24.8 ± 2.5% (n = 7 reactions) as determined with high-performance liquid chromatography, and the radiochemical purity of the final product was 93.0 ± 3.9% (n = 7 reactions). The specific activity of [^18^F]FBEM-EM3106B, corrected to EOB, ranged from 75.3 to 139.1 GBq/μmol (from 2.1 to 3.7 Ci/μmol).

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=21800885%5Buid%5D&cmd=DetailsSearch)]

An anti-GLP-1R antibody was used for the immunofluorescence staining of the pancreas as well as INS-1 cell xenograft tumors (insolinoma tumors; these cells express high levels of GLP-1R, see below) and MDA-MB-435 cell xenograft tumors obtained from nude mice (7). Microscopic examination of the tissues showed that the fluorescence signal was randomly distributed in the pancreas (because the β-cells that express the GLP-1R are unevenly distributed in the organ), that the INS-1 tumor cells showed intense fluorescent staining, and that the MDA-MB-435 cells (express very low levels of the GLP-1R) had a weak fluorescent signal.

Using ^125^I-GLP-1(7–36) as the radioligand, a competitive binding assay was performed with INS-1 cells. The 50% inhibition concentration values for EM3106B, FBEM-EM3106B, and GLP-1 were determined to be 1.25 ± 0.37 nM, 1.07 ± 0.84 nM, and 4.92 ± 0.58 nM, respectively (7). This indicated that EM3106B had a higher affinity for the receptor compared with GLP-1, and the conjugation of FBEM to EM3106B did not affect its binding affinity for GLP-1R. From a saturation binding assay with INS-1 cells and ^125^I-GLP-1(7–36) as the radiolabeled ligand, it was determined that the maximal binding for these cells was 6.8 × 10^3^ binding sites/cell (7).

The uptake, internalization, and efflux of [^18^F]-FBEM-EM3106B from INS-1 cells was investigated for up to 120 min after exposure to the tracer (7). The uptake of radioactivity in the cells after 15, 30, 60, and 120 min incubation was reported to be 1.91 ± 0.21% of total added dose (% AD), 2.94 ± 0.21% AD, 4.20 ± 0.23% AD, and 5.25 ± 0.61% AD, respectively. At 60 min and 120 min after incubation, the internalization of radioactivity was 3.17 ± 0.3% AD and 3.83 ± 0.55% AD, respectively. Incubation of the cells with [^18^F]-FBEM-EM3106B in the presence of unlabeled EM3106B (0.1 M) decreased the uptake to ~1.2% AD after 120 min, indicating that the probe bound specifically to the GLP-1R. Incubation of labeled cells in serum-free medium without the labeled ligand for various time periods (5 min to 2 h) showed that after a 2 h incubation ~50% of the radioactivity had dissociated and effluxed from the cells.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=21800885%5Buid%5D&cmd=DetailsSearch)]

For microPET imaging, nude mice bearing INS-1 or MDA-MB-435 cell xenograft tumors (under anesthesia; n = 6 animals/group) were injected with 3.7 MBq (100 μCi)/~100 to 200 nmol) [^18^F]-FBEM-EM3106B through the tail vein, and static PET images were acquired at 1 h and 2 h postinjection (p.i.) (7). The INS-1 tumors were clearly visible in the PET images at 1 h p.i., and the amount of radioactivity in the lesions was calculated to be 28.54 ± 4.74% of injected dose per gram tissue (% ID/g). By comparison, the uptake of label in the MDA-MB-435 cell tumors was 1.2% ID/g. To confirm the in vivo receptor binding specificity of [^18^F]-FBEM-EM3106B, nude mice bearing INS-1 cell xenograft tumors (n = 4 animals) were injected with the tracer in the presence of ~61 nmol unlabeled exendin-4, and static PET images of the rodents were acquired at 1 h p.i. Under these conditions, the uptake of radioactivity in the INS-1 tumors was significantly lower (~1.5% ID/g; P < 0.001) than that in the unblocked tumors (28.54 ± 4.74% ID/g), indicating that [^18^F]-FBEM-EM3106B had a high binding specificity for the GLP-1R. A high accumulation of radioactivity was observed in the liver (8.56 ± 1.61% ID/g) and kidneys (13.94 ± 1.79% ID/g), indicating that the tracer was excreted through the hepatobiliary and urinary routes in these animals.

To confirm observations made from the PET images, the biodistribution of radioactivity in various tissues from mice bearing INS-1 tumors was determined immediately after PET imaging (7). At 2 h p.i., the amount of radioactivity detected in the INS-1 tumor was 28.32 ± 3.91% ID/g, which was similar to the amount calculated from the PET images. The uptake values of label in the liver, kidneys, and pancreas at 2 h p.i. were 11.92 ± 1.75% ID/g, 29.18 ± 5.14% ID/g, and 5.45 ± 0.29% ID/g, respectively. The tumor/pancreas ratio was ~5, indicating that PET imaging with [^18^F]-FBEM-EM3106B can easily distinguish an insulinoma from the surrounding normal pancreatic tissue. Other organs, such as the stomach, intestine, spleen, muscle, and heart, showed accumulation values <5% ID/g. In the blocking study, a significantly reduced amount of radioactivity was detected in the tumor (1.10 ± 0.20% ID/g; P < 0.001) as compared with the PET images. A similar trend was apparent in the spleen, intestine, stomach, and other organs of the animals administered with a blocking dose of unlabeled exendin-4.

From these studies, the investigators concluded that [^18^F]-FBEM-EM3106B was potentially suitable for PET imaging of insulinomas in rodents (7).

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=21800885%20&cmd=DetailsSearch)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=21800885%20&cmd=DetailsSearch)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=21800885%20&cmd=DetailsSearch)]

No publication is currently available.

## Supplemental Information

[Disclaimers]

No information is currently available.

## NIH Support

Part of the work presented in this chapter was supported by the Intramural Research Program (IRP) of the National Institute of Biomedical Imaging and Bioengineering (NIBIB), National Institutes of Health.

## References

1 Batcher E., Madaj P., Gianoukakis A.G. (2011). Pancreatic neuroendocrine tumors. Endocr Res.
2 Mathur A., Gorden P., Libutti S.K. (2009). Insulinoma. Surg Clin North Am.
3 McAuley G., Delaney H., Colville J., Lyburn I., Worsley D., Govender P., Torreggiani W.C. (2005). Multimodality preoperative imaging of pancreatic insulinomas. Clin Radiol.
4 Wild D., Macke H., Christ E., Gloor B., Reubi J.C. (2008). Glucagon-like peptide 1-receptor scans to localize occult insulinomas. N Engl J Med.
5 Kiesewetter D.O., Gao H., Ma Y., Niu G., Quan Q., Guo N., Chen X. (2012). (18)F-radiolabeled analogs of exendin-4 for PET imaging of GLP-1 in insulinoma. Eur J Nucl Med Mol Imaging.
6 Wild D., Behe M., Wicki A., Storch D., Waser B., Gotthardt M., Keil B., Christofori G., Reubi J.C., Macke H.R. (2006). [Lys40(Ahx-DTPA-111In)NH2]exendin-4, a very promising ligand for glucagon-like peptide-1 (GLP-1) receptor targeting. J Nucl Med.
7 Gao H., Niu G., Yang M., Quan Q., Ma Y., Murage E.N., Ahn J.M., Kiesewetter D.O., Chen X. (2011). PET of insulinoma using 18F-FBEM-EM3106B, a new GLP-1 analogue. Mol Pharm.
8 Murage E.N., Gao G., Bisello A., Ahn J.M. (2010). Development of potent glucagon-like peptide-1 agonists with high enzyme stability via introduction of multiple lactam bridges. J Med Chem.
9 Kiesewetter D.O., Jacobson O., Lang L., Chen X. (2011). Automated radiochemical synthesis of [18F]FBEM: a thiol reactive synthon for radiofluorination of peptides and proteins. Appl Radiat Isot.

1. Batcher, E., P. Madaj, and A.G. Gianoukakis, Pancreatic neuroendocrine tumors. Endocr Res, 2011. 36(1): p. 35-43.

2. Mathur, A., P. Gorden, and S.K. Libutti, Insulinoma. Surg Clin North Am, 2009. 89(5): p. 1105-21.

3. McAuley, G., H. Delaney, J. Colville, I. Lyburn, D. Worsley, P. Govender, and W.C. Torreggiani, Multimodality preoperative imaging of pancreatic insulinomas. Clin Radiol, 2005. 60(10): p. 1039-50.

4. Wild, D., H. Macke, E. Christ, B. Gloor, and J.C. Reubi, Glucagon-like peptide 1-receptor scans to localize occult insulinomas. N Engl J Med, 2008. 359(7): p. 766-8.

5. Kiesewetter, D.O., H. Gao, Y. Ma, G. Niu, Q. Quan, N. Guo, and X. Chen, (18)F-radiolabeled analogs of exendin-4 for PET imaging of GLP-1 in insulinoma. Eur J Nucl Med Mol Imaging, 2012. 39(3): p. 463-73.

6. Wild, D., M. Behe, A. Wicki, D. Storch, B. Waser, M. Gotthardt, B. Keil, G. Christofori, J.C. Reubi, and H.R. Macke, [Lys40(Ahx-DTPA-111In)NH2]exendin-4, a very promising ligand for glucagon-like peptide-1 (GLP-1) receptor targeting. J Nucl Med, 2006. 47(12): p. 2025-33.

7. Gao, H., G. Niu, M. Yang, Q. Quan, Y. Ma, E.N. Murage, J.M. Ahn, D.O. Kiesewetter, and X. Chen, PET of insulinoma using 18F-FBEM-EM3106B, a new GLP-1 analogue. Mol Pharm, 2011. 8(5): p. 1775-82.

8. Murage, E.N., G. Gao, A. Bisello, and J.M. Ahn, Development of potent glucagon-like peptide-1 agonists with high enzyme stability via introduction of multiple lactam bridges. J Med Chem, 2010. 53(17): p. 6412-20.

9. Kiesewetter, D.O., O. Jacobson, L. Lang, and X. Chen, Automated radiochemical synthesis of [18F]FBEM: a thiol reactive synthon for radiofluorination of peptides and proteins. Appl Radiat Isot, 2011. 69(2): p. 410-4.